# Superparamagnetic iron oxide nanoparticles (SPION) stabilized by alginate

Chemical name: | Superparamagnetic iron oxide nanoparticles (SPION) stabilized by alginate
Abbreviated name: | SPION-alginate
Synonym: | SPIO-alginate
Agent Category: | Nanoparticles
Target: | Reticuloendothelial system (RES)
Target Category: | Non-targeted (phagocytosis)
Method of detection: | Magnetic resonance imaging (MRI)
Source of signal / contrast: | Superparamagnetic iron oxide (SPIO)
Activation: | No
Studies: | - In vitro; - Rodents | No structure available

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=superparamagnetic%20iron%20oxide%20and%20imaging)]

Superparamagnetic iron oxide nanoparticles (SPION) stabilized by alginate (SPION-alginate) have been developed as a contrast agent to improve the sensitivity of magnetic resonance imaging (MRI) in the detection of hepatocellular carcinoma (HCC) (1-3).

MRI is an imaging modality that is used to construct images of the nuclear magnetic resonance (NMR) signal, primarily from the hydrogen atoms in an object. The image contrast is achieved by the differences in the NMR signal intensity in different areas within the object, and the NMR signal intensity largely depends on the nuclear density (proton spins), the relaxation times (T_1_, T_2_, and T_2_*), and the magnetic environment of the tissues. Contrast agents serve to enhance the image contrast, thus improving the sensitivity and specificity of MRI in mapping information from tissues (4, 5). SPION comprise a class of novel MRI contrast agents that are composed of a ferric iron (Fe^3+^) and ferrous iron (Fe^2+^) core and a layer of dextran or other polysaccharide coating (4, 6). The iron nanoparticles have very large magnetic moment, which leads to local magnetic field inhomogeneity. Consequently, the NMR signal intensity is significantly decreased, appearing dark on T_2_- and T_2_*-weighted images. On the basis of size (i.e., diameter), SPION are commonly classified as oral SPIO (300 nm–3.5 µm), polydisperse SPIO (PSPIO, 50–150 nm), and ultrasmall SPIO (USPIO, <50 nm). In addition, USPIO nanoparticles with an iron oxide core that is monocrystalline in nature are referred to as monocrystalline iron oxide nanoparticles (MION), and MION with a chemically cross-linked and aminated polysaccharide shell are called cross-linked iron oxide nanoparticles (CLIO) (7).

SPION are predominantly used as a T_2_/T_2_* contrast agent in the clinic, though it could shorten both T_1_ and T_2_/T_2_* relaxation processes. Successful application of a SPION-based contrast agent is dependent on its size, size distribution, shape, magnetic susceptibility, and surface modification. In vivo, nonspecific SPION are mainly captured by the reticuloendothelial system, and they are more suitable for liver, spleen, and lymph node imaging (8). Because of the long plasma half-life (hours), they are also used as blood pool agents in magnetic resonance angiography (9). Specific SPION are developed by conjugating the respective targeting agents directly onto the SPION surface or onto its hydrophilic coating. Specific accumulation of the agents at disease-specific sites is achieved because of the target overexpression (often cell surface receptors) and receptor-mediated endocytosis and recycling (4, 5). The signal decrease is much more obvious in the lesions than in the surrounding normal tissues. An inverse strategy of the SPION-based molecular imaging is also applied in some studies by designing molecules that bind to targets expressing on normal tissues. This strategy has been proved to be valuable in imaging pancreatic ductal adenocarcinomas and HCC by targeting the receptors of bombesin, cholecystokinin, or asialoglycoprotein (10, 11). In this case, by decreasing the T_2_ signal of normal tissue surrounding a tumor more than that of the tumor, the contrast between healthy and tumor tissues is enhanced.

A SPION-based MRI contrast agent was developed by stabilizing the SPION with alginate (SPION-alginate) (1-3). In vivo application of this newly developed contrast agent improved the sensitivity of MRI in the detection of HCC in rat and rabbit HCC models.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=superparamagnetic%20iron%20oxide%20and%20alginate%20and%20MRI)]

The contrast agent SPION-alginate was prepared with a two-step coprecipitation method as a formation of Fe_3_O_4_ by coprecipitation of ferric and ferrous ion with alkaline solution and stabilization of the SPION with alginate polymer (2). Briefly, ferric and ferrous chlorides were first dissolved in distilled water, followed by precipitation with NaOH solution at 60ºC. Sodium alginate solution was then added to the suspension containing the Fe_3_O_4_ nanoparticles with vigorous stirring for 30 min. The mixture was first heated for 1 h at 80ºC with slow stirring, and then it was sonicated for 20 min. The solution was dialyzed against deionized water to remove the FeCl_2_ and FeCl_3_ and then centrifuged to remove the solid materials. The supernatant containing SPION-alginate was collected (used as suspension sample), and a fraction of the supernatant was dried with a rotary evaporator at 50ºC to obtain a solid sample. Three kinds of sodium alginate were tested separately to stabilize the SPION, including Keltone LVCR (54 kDa, M/G ratio 1.5), Keltone HVCR (160 kDa, M/G ratio 1.5), and Manugel DMB (124 kDa, M/G ratio 0.6). All the above processes were run under N_2_ protection. The Fe_3_O_4_ contents in the solid samples varied with the types of alginate but changed little with different concentrations of alginate (LVCR, 1–4% (w/w)). With 1% LVCR, the Fe_3_O_4_ content reached up to 50% (w/w). In the suspension samples, the Fe_3_O_4_ concentrations were 1–4 mg/ml when coated or stabilized with LVCR alginate (1–4%, w/w), two-fold higher than concentrations when coated with HVCR or DMB.

X-ray diffraction analysis confirmed that the nanoparticles were Fe_3_O_4_ with an average diameter of 2.6 nm. Under electronic microscopy, the Fe_3_O_4_ nanoparticles were cube-shaped and monodispersed with a diameter of ~10 nm. The Fe_3_O_4_-alginate looked like a sponge with Fe_3_O_4_ nanoparticles embedded in the alginate substrate. The average hydrodynamic radius of the SPION-alginate was 193.8–483.2 nm, increasing with increased concentrations of alginate (1–4%, w/w). It has been assumed that the polydispersity of alginate is responsible for the large size of SPION-alginate because the Z-average hydrodynamic radius of the pure alginate solution was 200–500 nm. Under atomic force microscopy, the SPION-alginate appeared as a bright spot in liquid with an average diameter of 4.678 nm for the Fe_3_O_4_ core. In air, the Fe_3_O_4_ nanoparticles bound to the strands of alginate macromolecules with an average diameter of 7.530 nm, larger than in liquid. The binding of Fe_3_O_4_ with alginate was also confirmed with Fourier transform infrared spectroscopy, showing a specific shift of the frequencies in the spectra of SPION-alginate. The ξ-potentials of the SPION-alginate coated with LVCR alginate at 1–4% (w/w) ranged from −57.0 to −75.7 mV, similar to the ξ-potential of the alginate solution (−71.8 mV). No sedimentation was observed in bottles of the SPION-alginate filled with nitrogen gas even after 12 months of storage at 4ºC at pH 7.0, indicating that the SPION-alginate nanoparticles were highly stable.

The magnetic property of the SPION-alginate was investigated at 300 K. Magnetization did not reach saturation, even at the applied magnetic field strength of 10,000 oersted (Oe) and no hysteresis was found. These data indicated that the nanoparticles were superparamagnetic. The saturation magnetization (Ms) of the solid samples with 12.5% and 47.0% Fe_3_O_4_ was 55 and 52 emu/g, respectively, while the Ms of corresponding suspension samples with 1.09 and 3.02 mg/ml Fe_3_O_4_ was 40 and 38 emu/g, respectively. The Ms of the solution samples was 73% of the Ms of the solid samples. In T_1_-weighted images, the signal intensity of the SPION-alginate was stronger, and in T_2_-weighted images, the signal was weaker than that of the saline. With increased Fe_3_O_4_ concentrations of 0.074–0.300 mmol, T_1_ relaxation time decreased from 1,450 to 400 ms and T_2_ relaxation time decreased from 40 to 10 ms. The T_1_ and T_2_ relaxivities of the SPION-alginate in saline (1.5 T, 20ºC) were 7.9 ± 0.2 and 281.2 ± 26.4 mM−^1^ s−^1^, respectively. The relative magnitude of T_1_ and T_2_ relaxivities was 35.7, suggesting that the SPION-alginate nanoparticles had a moderate T_1_ shortening effect and a strong T_2_ shortening effect.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=superparamagnetic%20iron%20oxide%20and%20alginate%20and%20MRI)]

Ma et al. analyzed the potential adverse effect of the SPION-alginate on red blood cells and cytotoxicity to L929 cells (mouse fibroblasts) and RAW264.7 cells (mouse macrophages) (1, 3). L929 cells are widely used as the reference cells for polymer cytotoxicity analysis, and RAW264.7 cells are commonly used for cell uptake testing of SPION. Incubation of the rabbit erythrocytes with up to 0.57 mg Fe/ml SPION-alginate for 3 h at 37ºC did not result in evident hemolysis (<5%). No erythrocyte aggregation was observed after 1 h incubation at 37ºC. The cell growth of neither L929 nor RAW264.7 cells was inhibited upon exposure of 6.125–100 µg Fe/ml SPION-alginate for 24 h. After 24 h incubation with 12.5–50.0 µg Fe/ml SPION-alginate, almost all RAW264.7 cells were labeled with the SPION-alginate, presenting abundant Fe_3_O_4_ nanoparticles in the cytoplasm. The internalization was dependent on both Fe_3_O_4_ concentration and time.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=superparamagnetic%20iron%20oxide%20and%20alginate%20and%20MRI)]

The pharmacokinetics of the SPION-alginate was investigated in healthy male Sprague-Dawley rats after intravenous administration (1, 3). Twenty-nine rats were used for whole-blood studies by dividing the rats into a low-dose group (109.5 µmol Fe/kg, n = 18 rats), a high-dose group (218.9 µmol Fe/kg, n = 3 rats), an alginate-alone group (n = 3 rats), and a physiological saline group (n = 5 rats). An additional 20 rats were set for serum studies (n = 5/group). Ex vivo whole-blood studies showed that the blood iron reached the maximum level at 5 min, followed by a gradual decrease to the lowest level at 48 h after injection (from 515.5 to 266.3 µg/ml for the low-dose group, and from 647.7 to 333.6 µg/ml for the high-dose group). The blood iron level returned to the baseline (~471.9 µg/ml before injection) at 96 h after injection. In the rats given alginate alone or saline, the patterns of blood iron level changes were similar, mildly decreased at first and recovered later. However, the blood iron levels in all rats were lower than the baseline up to 48 h after injection of alginate alone or saline. The baseline serum iron level fluctuated between 6.06 and 15.22 µg/mmol. After injection of the SPION-alginate, the serum iron level increased rapidly and then decreased to the baseline at 3 h for the low-dose group and at 6 h for the high-dose group. The half-life of the SPION-alginate was 0.27 ± 0.06 h at the low-dose and 0.65 ± 0.22 h at the high-dose. The serum iron concentration change over time after injection of the SPION-alginate were provided in table 1 by Ma et al. (3), however the relationship between the injected does and the iron amount in serum were not described.

Tissue distribution studies showed that the iron levels in the liver and spleen increased markedly after intravenous injection of low-dose SPION-alginate. More than 80% of the injected iron accumulated in the liver, and ~10% accumulated in the spleen. The iron accumulation peaked at 30 min in the liver (235.05 ± 19.62 µg Fe/kg) and at 24 h in the spleen (402.28 ± 187.31 µg Fe/kg). The iron elimination was slower from the liver than from the spleen. Less than 2% of the injected iron accumulated in the lungs, heart, and kidneys. Staining of the liver and spleen tissues demonstrated that the iron accumulated in the Kupffer cells of the hepatic sinusoid and in the cord and red pulp of the spleen at 30 min to 14 days after injection. At 30 min, the iron particles were found to be mainly distributed in the peripheral region of the hepatic lobules, and in the center region at 96 h. The iron particles were still observable at 14 days after injection.

MRI was performed with a 3.0-T MR scanner in healthy male Sprague-Dawley rats (n = 6), rats with diethylnitrosoamine-induced primary liver cancer (n = 29), and rabbits transplanted with VX2 tumor. The signal/noise ratio (SNR) was calculated by dividing the signal intensity by the standard deviation of noise. The contrast/noise ratio (CNR) was calculated with the following formula: (signal intensity of the HCC – signal intensity of the cirrhotic liver tissue)/standard deviation of noise. In healthy rats, the SNR in the liver decreased at 10 min and remained stable up to 180 min after injection. For the rat primary tumor model, 15 rats survived at week 18 of experiments and were used for MRI studies. All 15 rats were accompanied by severe hepatic cirrhosis, and no HCC was found with MRI in any rat before injection of the SPION-alginate. Interestingly, 22 HCCs were found in 11 rats after injection of the SPION-alginate, and the other 4 rats were diagnosed with simple cirrhosis. The SNR in the healthy liver tissue decreased from 48.95 ± 4.87 before injection to 6.43 ± 3.37 after injection, and in the cirrhotic tissue it decreased from 45.51 ± 11.71 to 23.47 ± 7.52. There was no marked change for the SNR in the HCC (45.51 ± 11.71 before injection and 40.53 ± 12.98 after injection). Are they looking simply at SPION? The HCC should be much lower if they are looking at SPION; it looks like they are looking at other sources of iron? The CNR of the HCC increased from 0 before injection to 17.69 ± 3.69 after injection. The contrast between HCC and liver parenchyma was significantly increased. With Perls staining of the tissues after MRI, the SPION were observed in the normal liver parenchyma, hyperplastic nodules, and hemangiomas, but not in the HCC. MRI with SPION alone was not performed for comparison of the contrast enhancement between SPION-alginate and SPION alone.

Similar results were obtained with the MRI studies on the rabbit VX2 tumor model. The MRI signal intensity in the liver parenchyma decreased, but did not decrease in the VX2 tumor. The borderline of the tumor was more obvious in comparison with that of unenhanced images. Perls staining again showed that the SPION were present in the normal part of the liver but not in the tumor.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22%20SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Ma H.L., Qi X.R., Ding W.X., Maitani Y., Nagai T. (2008). Magnetic targeting after femoral artery administration and biocompatibility assessment of superparamagnetic iron oxide nanoparticles. J Biomed Mater Res A.
2 Ma H.L., Qi X.R., Maitani Y., Nagai T. (2007). Preparation and characterization of superparamagnetic iron oxide nanoparticles stabilized by alginate. Int J Pharm.
3 Ma H.L., Xu Y.F., Qi X.R., Maitani Y., Nagai T. (2008). Superparamagnetic iron oxide nanoparticles stabilized by alginate: pharmacokinetics, tissue distribution, and applications in detecting liver cancers. Int J Pharm.
4 Islam T., Josephson L. (2009). Current state and future applications of active targeting in malignancies using superparamagnetic iron oxide nanoparticles. Cancer Biomark.
5 Corot C., Robert P., Idee J.M., Port M. (2006). Recent advances in iron oxide nanocrystal technology for medical imaging. Adv Drug Deliv Rev.
6 Bulte J.W., Kraitchman D.L. (2004). Iron oxide MR contrast agents for molecular and cellular imaging. NMR Biomed.
7 Di Marco M., Sadun C., Port M., Guilbert I., Couvreur P., Dubernet C. (2007). Physicochemical characterization of ultrasmall superparamagnetic iron oxide particles (USPIO) for biomedical application as MRI contrast agents. Int J Nanomedicine.
8 Tanimoto A., Kuribayashi S. (2006). Application of superparamagnetic iron oxide to imaging of hepatocellular carcinoma. Eur J Radiol.
9 Maes R.M., Lewin J.S., Duerk J.L., Misselwitz B., Kiewiet C.J., Wacker F.K. (2006). A new type of susceptibility-artefact-based magnetic resonance angiography: intra-arterial injection of superparamagnetic iron oxide particles (SPIO) A Resovist in combination with TrueFisp imaging: a feasibility study. Contrast Media Mol Imaging.
10 Tanimoto A., Kuribayashi S. (2005). Hepatocyte-targeted MR contrast agents: contrast enhanced detection of liver cancer in diffusely damaged liver. Magn Reson Med Sci.
11 Montet X., Weissleder R., Josephson L. (2006). Imaging pancreatic cancer with a peptide-nanoparticle conjugate targeted to normal pancreas. Bioconjug Chem.